# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7,10-tetraacetic acid-cyclo(CGNSNPKSC)

Chemical name: | ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-cyclo(CGNSNPKSC)
Abbreviated name: | ^64^Cu-DOTA-GX1
Synonym:
Agent category: | Peptide
Target: | Tumor vasculature
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1)]

Angiogenesis is an essential process in the development of new blood vessels in normal physiological states and in diseases (1, 2). Targeting of tumor vasculature is a promising strategy for tumor imaging and therapy because tumor growth and metastasis largely depend on angiogenesis (3, 4). A cyclic 9-mer peptide (CGNSNPKSC (GX1)) was initially identified as a recognition motif for binding to the human gastric tumor vasculature (5-7). GX1 has also been shown to bind to a variety of human cancer vasculatures. The molecular target of GX1 has not been identified; however, GX1 inhibits endothelial cell proliferation in vitro and neovascularization in vivo. The Lys (K) residue of GX1 was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in mice bearing U89MG human glioblastoma tumors (8). Cy5.5-GX1 exhibited high near-infrared fluorescence intensity in U89MG tumors in nude mice. For positron emission tomography (PET) imaging, ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-GX1 (^64^Cu-DOTA-GX1) was prepared and evaluated in nude mice bearing U89MG tumors (9).

### Related Resource Links:

- Chapters in MICAD (GX1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GX1+AND+micad%5Bbook%5D))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+synthesis)]

The Boc-protected GX1 peptide was obtained using solid-phase synthesis. DOTA-N-hydroxysuccinimide (NHS) ester (1,193 nmol) was used to conjugate the peptide (994 nmol) for 2 h at 45°C (9). The NHS ester of DOTA reacted with the Ɛ-amino group of the Lys residue of the peptide. The Boc-protected DOTA-GX1 was isolated with high-performance liquid chromatography (HPLC), with 87% yield. Trifluoracetic acid was used to remove the Boc-protecting group to form DOTA-GX1, with 85% yield and >97% chemical purity after HPLC purification. Mass spectroscopy analysis confirmed a 1:1 addition of DOTA to GX1. DOTA-GX1 (5 nmol) was incubated with 37–111 MBq (1–3 mCi) ^64^CuCl_2_ in ammonium acetate buffer (pH 5.5) for 30 min at 45°C. ^64^Cu-DOTA-GX1 was purified with high-performance liquid chromatography. This procedure provided a radiolabeling yield of >90%, with a specific activity of 37 GBq/µmol (1 Ci/µmol) and a radiochemical purity of >99%. ^64^Cu-DOTA-GX1 was 95% and 91% intact for 6 h and 24 h, respectively, at 37°C in phosphate-buffered saline (PBS). Log P (pH 7.4) for ^64^Cu-DOTA-GX1 in PBS was determined to be −2.42 (rather hydrophilic).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+and+in+vitro)]

Flow cytometry analysis showed that 6%, 12%, and 25% of U89MG cells (1.5 × 10^6^) were positive after incubation with 0.5, 1, and 4 nmol Cy5.5-GX1 for 60 min at 4°C (8). Confocal microscopy showed internalization of fluorescence activity inside the cells. No blocking studies were performed with unlabeled GX1.

Chen et al. (9) showed that the cellular accumulation of radioactivity was 0.10% and 0.29% incubation dose (ID) at 1 h and 2 h after incubation of U89MG cells (0.25 × 10^6^) with ^64^Cu-DOTA-GX1 at 37°C. Efflux study showed that >75% of radioactivity was retained after 2 h incubation in fresh medium. Neither the binding affinity nor in vitro blocking studies were performed with unlabeled GX1.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+rodentia)]

Chen et al. (9) performed PET imaging in nude mice (n = 3) bearing U89MG tumors at 0.5, 1, 15, 24, and 39 h after injection of 5.55 MBq (0.15 mCi) ^64^Cu-DOTA-GX1. The tumors were clearly visualized at 0.5 h. The tumor accumulation values were 3.01 ± 0.53%, 3.20 ± 0.54%, 5.43 ± 0.40%, 7.97 ± 0.75%, and 5.20 ± 0.44% injected dose/gram (ID/g) at 0.5, 1, 15, 24, and 39 h, respectively. The liver and kidney accumulation values were 17.81 ± 0.30% ID/g and 17.87 ± 0.30% ID/g at 0.5 h, respectively. The radioactivity was steadily cleared from the liver and kidneys, with 1.61 ± 0.16% and 1.11 ± 0.09% at 39 h, respectively. The highest tumor contrast was observed at 24 h. Co-injection of GX1 (20 µmol/kg) inhibited the tumor accumulation by 75% at 24 h after injection (P < 0.01), with significant inhibition (40%–50%) in the liver and kidneys. ^64^Cu-DOTA-GX1 was 75%, 82%, 38%, and 64% intact in the blood, urine, liver, and kidneys, respectively, at 1 h after injection in a normal nude mouse.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GX1+human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Carmeliet P. (2004). Manipulating angiogenesis in medicine. J Intern Med.
2 Folkman J. (2007). Angiogenesis: an organizing principle for drug discovery?. Nat Rev Drug Discov.
3 Abdollahi A., Folkman J. (2010). Evading tumor evasion: current concepts and perspectives of anti-angiogenic cancer therapy. Drug Resist Updat.
4 Thorpe P.E. (2004). Vascular targeting agents as cancer therapeutics. Clin Cancer Res.
5 Chen B., Cao S., Zhang Y., Wang X., Liu J., Hui X., Wan Y., Du W., Wang L., Wu K., Fan D. (2009). A novel peptide (GX1) homing to gastric cancer vasculature inhibits angiogenesis and cooperates with TNF alpha in anti-tumor therapy. BMC Cell Biol.
6 Hui X., Han Y., Liang S., Liu Z., Liu J., Hong L., Zhao L., He L., Cao S., Chen B., Yan K., Jin B., Chai N., Wang J., Wu K., Fan D. (2008). Specific targeting of the vasculature of gastric cancer by a new tumor-homing peptide CGNSNPKSC. J Control Release.
7 Zhi M., Wu K.C., Dong L., Hao Z.M., Deng T.Z., Hong L., Liang S.H., Zhao P.T., Qiao T.D., Wang Y., Xu X., Fan D.M. (2004). Characterization of a specific phage-displayed Peptide binding to vasculature of human gastric cancer. Cancer Biol Ther.
8 Chen, K., L.P. Yap, R. Park, X. Hui, K. Wu, D. Fan, X. Chen, and P.S. Conti, A Cy5.5-labeled phage-displayed peptide probe for near-infrared fluorescence imaging of tumor vasculature in living mice. Amino Acids, 2011
9 Chen K., Sun X., Niu G., Ma Y., Yap L.P., Hui X., Wu K., Fan D., Conti P.S., Chen X. (2012). Evaluation of (64)Cu Labeled GX1: A Phage Display Peptide Probe for PET Imaging of Tumor Vasculature. Mol Imaging Biol.